# Evans Blue-diethylenetriamine-N,N,N”,N”-pentaacetic acid-gadolinium

Chemical name: | Evans Blue-diethylenetriamine-N,N,N”,N”-pentaacetic acid-gadolinium
Abbreviated name: | EB-DTPA-Gd
Synonym:
Agent Category: | Compound
Target: | Vascular lesions
Target Category: | Nonspecific binding to proteins
Method of detection: | Magnetic resonance imaging (MRI)
Source of signal: | Gd
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=EB-DTPA-Gd)]

Endothelium, the inner lining of blood vessels, is considered to be the largest organ of the animal body, and its major function, including the secretion of several bioactive molecules, is to maintain vascular homeostasis (1, 2). Any disruption of the normal epithelium functions or the formation of a lesion as a result of shear stress, pressure, cellular metabolism, or other unknown factors can trigger localized inflammation or the development of atherosclerotic plaques at the site of disruption (3). Therefore, early detection and determination of the degree of vascular injury is important for the development of a therapeutic regimen for this condition. Detection of the plaques in human coronary arteries is particularly important because, if left untreated, such plaques can result in myocardial infraction and even death. A variety of techniques, including computed tomography and magnetic resonance imaging (MRI), and different imaging agents linked to antibodies against proteins related to vascular disease have been designed and are now used to detect atherosclerotic plaques (4). However, most of these methods and agents are expensive and complicated to produce. Yamamoto et al. developed and evaluated an MRI contrast agent using a readily available and inexpensive dye, Evans Blue (EB), that could be used specifically to view vascular lesions (5). EB is a di-azo dye that has been used extensively for the determination of cell membrane permeability and blood volume in animals (6, 7). An MRI agent was generated by the conjugation of EB to diethylenetriamene pentaacetic acid (DTPA) to facilitate the binding of gadolinium (Gd) to obtain EB-DTPA-Gd, the contrast agent used in studies reviewed in this chapter (5, 8, 9).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=EB-DTPA-Gd+synthesis)]

The synthesis of EB-DTPA-Gd was described by Yamamoto et al. (5). To start, 2,2’-dimethylbenzidine (DMB) was dissolved in dichloromethane, and di-tertiary-butyl dicarbonate was added to it dropwise at room temperature with stirring. The reaction was allowed to proceed overnight, and excess DMB was removed with an aqueous saturated solution of tartaric acid. The organic phase was vacuum-concentrated, and the residue was purified with silica gel column chromatography to obtain N-tertiary butoxycarbonyl-DMB as a pale yellow solid. The yield of this reaction was 43%.

To synthesize the DTPA derivative of N-tertiary butoxycarbonyl-DMB, the two chemicals were dissolved in dimethylsulfoxide and the mixture was stirred at 40°C for 3 h. The resulting mixture was then poured into cold water, and the precipitate was collected by filtration. The precipitate was dissolved in sodium bicarbonate (pH 7.0) and purified with octadecylsilyl column chromatography. The appropriate fractions were pooled and freeze-dried to obtain a solid. The solid was dissolved in trifluoroacetic acid (TFA) and stirred at room temperature for 1 h. This solution was poured into cold ether, and the resulting precipitate was collected by filtration. The precipitate was then dried under vacuum to obtain DMB-DTPA 4TFA, a colorless solid. The yield of this reaction was 14%.

To obtain the DTPA derivative of EB, DMB-DTPA 4TFA was dissolved in water containing hydrochloric acid (HCl) and mixed with sodium nitrate for 20 min. This solution was then mixed for 3 h with sodium bicarbonate in a 1-amino-8-naphtol-2,4-disulfonic acid solution. The reaction mixture was freeze-dried, and the residue was dissolved in water. EB-DTPA was precipitated from the solution by mixing it with concentrated HCl. The yield of this reaction was 81%. The precipitate was collected and dried under vacuum.

To obtain the MRI contrast agent, equimolar solutions of gadolinium chloride (GdCl_3_) and EB-DTPA were mixed. The pH of this solution was adjusted to 7.0 with sodium hydroxide. The solution was then lyophilized to obtain the contrast agent as a solid. Conditions for storage and stability of the contrast agent were not reported by the investigators (5).

The EB-DTPA used in some studies was synthesized as detailed above. Although DTPA-Gd was used in some studies, its synthesis or procurement from a commercial source was not reported by the investigators (5, 8, 9).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=EB-DTPA-Gd+tissue)]

The use of EB-DTPA-Gd for the detection of vascular injury was evaluated in vitro with a porcine aorta section (5). The porcine aorta was opened flat, and the endothelium on the left half of the center axis was scraped with a scalpel while the right half was left intact. The entire aorta section was then dipped in a solution of EB-DTPA-Gd for 10 s and washed with saline. The aorta section was then evaluated with MRI. The T1-weighted MRI was reported to distinguish between the damaged and intact areas of the aorta, and MRI signal enhancement was observed only in the inner surface area of the aortic wall, indicating that the dye did not permeate into the tissue from the injured endothelium site (5). The MRI signal obtained with EB-DTPA-Gd was compared to that obtained with DTPA-Gd, and it was observed that the signal with DTPA-Gd was close to the background levels obtained with EB-DTPA-Gd. This was suggested to indicate that DTPA-Gd, compared to EB-DTPA-Gd, did not adsorb on the surface of the vascular lesion. The MRI signal was observed to increase with the concentration of EB-DTPA-Gd, and it was determined that a 10-mM concentration of EB-DTPA-Gd was sufficient to saturate the lesion area (5). At this concentration the MRI signal was 1.5 times that of the intact epithelium. It was also reported the signal could be obtained even in presence of serum (8).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=EB-DTPA-Gd+rodentia)]

A balloon injury in the left carotid artery of rats was created as described elsewhere (10). The EB-DTPA-Gd contrast solution was then injected into the animals through the jugular vein, and T1-weighted MR images of the carotid artery were obtained through the transaxial plane (8). The investigators reported a clear increase in the signal from the injured artery compared to an intact common artery image in the control artery. In addition, an increase in MRI intensity was not observed when DTPA-Gd was used as the imaging agent either in the intact or the injured artery. This indicated that EB-DTPA-Gd could also be used in an in vivo setting (8). In the same study, the right (normal for use as a control) and left (injured by ballooning) common carotid arteries were extracted from the rats at 10, 30, and 120 min after reagent injection. The arteries were then opened and fixed on a glass plate for ex vivo MRI analysis as described above (5). The MRI signal intensity was highest at 10 min; it gradually decreased with time and was reported to be down to levels similar those of the intact artery at 120 min after the injection. With the results obtained from this study, the investigators concluded that EB-DTPA-Gd could be used for the non-invasive detection of vascular injury (8).

The use of EB-DTPA-Gd for the MRI detection of atherosclerotic lesions in apolipoprotein-E–deficient mice (http://taconic.com/wmspage.cfm?parm1=901) (ApoE^-/-^ mice) was investigated by Yasuda et al. (9). ApoE^-/-^ mice of different ages (3 to 12 months) were used in the study (n = 3–4 animals in each group), and age-matched normal mice were used as controls. The animals were intravenously injected with EB-DTPA-Gd through the tail vein, and MRI of the aorta of the animals was performed between 0 and 30 min after administration of the dye. The signal intensity was significantly (P < 0.05) different between the ApoE^-/-^ (146 ± 33) and normal (62 ± 23) mice. In addition, an increase in intensity of the aortic wall signal was observed with an increase in age (P = 0.05). The investigators observed a correlation between the enhanced MRI signal and macroscopic location of the atherosclerotic lesion on the aorta as determined with Sudan Red staining (9). The investigators cautioned that, although the contrast agent appeared to be useful for non-invasive detection of atherosclerotic plaques, the in vivo bioactivity, specificity, and adverse effects of the agent remain to be investigated.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=EB-DTPA-Gd+Non-Primate+Mammals)]

No publications are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=EB-DTPA-Gd+Non-Human+Primates)]

No publications are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=EB-DTPA-Gd+Humans)]

No publications are currently available.

## References

1 Hartge M.M., Unger T., Kintscher U. (2007). The endothelium and vascular inflammation in diabetes. Diab Vasc Dis Res.
2 Tziomalos K., Athyros V.G., Karagiannis A., Mikhailidis D.P. (2007). Endothelial function, arterial stiffness and lipid lowering drugs. Expert Opin Ther Targets.
3 Vanepps J.S., Vorp D.A. (2007). Mechano-pathobiology of atherogenesis: a review. J Surg Res.
4 Briley-Saebo K.C., Mulder W.J., Mani V., Hyafil F., Amirbekian V., Aguinaldo J.G., Fisher E.A., Fayad Z.A. (2007). Magnetic resonance imaging of vulnerable atherosclerotic plaques: current imaging strategies and molecular imaging probes. J Magn Reson Imaging.
5 Yamamoto T., Ikuta K., Oi K., Abe K., Uwatoku T., Murata M., Shigetani N., Yoshimitsu K., Shimokawa H., Katayama Y. (2004). First functionalized MRI contrast agent recognizing vascular lesions. Anal Sci.
6 Hamer P.W., McGeachie J.M., Davies M.J., Grounds M.D. (2002). Evans Blue Dye as an in vivo marker of myofibre damage: optimising parameters for detecting initial myofibre membrane permeability. J Anat.
7 Davy K.P., Seals D.R. (1994). Total blood volume in healthy young and older men. J Appl Physiol.
8 Yamamoto T., Ikuta K., Oi K., Abe K., Uwatoku T., Hyodo F., Murata M., Shigetani N., Yoshimitsu K., Shimokawa H., Utsumi H., Katayama Y. (2004). In vivo MR detection of vascular endothelial injury using a new class of MRI contrast agent. Bioorg Med Chem Lett.
9 Yasuda S., Ikuta K., Uwatoku T., Oi K., Abe K., Hyodo F., Yoshimitsu K., Sugimura K., Utsumi H., Katayama Y., Shimokawa H. (2007). In vivo Magnetic Resonance Imaging of Atherosclerotic Lesions with a Newly Developed Evans Blue-DTPA-Gadolinium Contrast Medium in Apolipoprotein-E-Deficient Mice. J Vasc Res.
10 Uwatoku T., Shimokawa H., Abe K., Matsumoto Y., Hattori T., Oi K., Matsuda T., Kataoka K., Takeshita A. (2003). Application of nanoparticle technology for the prevention of restenosis after balloon injury in rats. Circ Res.